# ^99m^Tc-Labeled cysteine-tagged dimeric epidermal growth factor

Chemical name: | ^99m^Tc-Labeled cysteine-tagged dimeric epidermal growth factor
Abbreviated name: | [^99m^Tc]Cys-dEGF
Synonym:
Agent Category: | Ligand
Target: | Epidermal growth factor receptor (EGFR)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click here for the protein and nucleotide sequence (http://www.ncbi.nlm.nih.gov/nuccore/166362727?report=genbank) of human epidermal growth factor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=role+of+growth+factors+in+cancer)]

Growth factors such as the epidermal growth factor (EGF), the vascular endothelial growth factor (VEGF), and the tumor necrosis factor are known to have important roles in the development and progression of cancers (1-3). The EGF mediates its activity through a group of tyrosine kinase (TK)–dependent EGF receptors (EGFR) that promote not only cell proliferation but also cell survival and the motility phenotype that is necessary for the development of an invasive cancer (4). As a consequence, the EGFRs and their associated TKs are the targets of several anti-EGFR antibodies (http://clinicaltrials.gov/ct2/results?term=anti-EGFR+antibodies) and TK inhibitors (http://clinicaltrials.gov/ct2/results?term=EGFR+tyrosine+kinase+inhibitors) that are either approved by the United States Food and Drug Administration or are being evaluated in clinical trials for the treatment of various neoplasms. Before treatment, the patients are screened to determine the extent of EGFR expression in the tumors with the use of immunohistochemistry (IHC) or fluorescence in situ hybridization (FISH) because these techniques help predict the probable therapeutic response and outcome for the individual (5, 6). However, only 10–25% of the patients who are EGFR-positive according to IHC or FISH analysis respond to the anti-EGFR therapy, which indicates that a poor correlation exists between the EGFR expression analysis and the treatment (7, 8). This is probably because only the active receptors are important to predict the efficacy of the anti-EGFR agents for the treatment of cancers, and ICH and FISH do not distinguish between the active and inactive EGFRs (9).

On binding the ligand, a characteristic feature of a functional EGFR is that it is internalized by the cell. Levashova et al. (10) envisioned that perhaps the natural ligand EGF itself could be used as an imaging agent to detect the active EGFRs in tumors. The investigators used an Escherichia coli (E. coli)–expressed dimeric EGF (dEGF) molecule in which the second EGF molecule is linked to the first through a linker of 9 amino acids, with the first EGF molecule having an N-terminal cysteine fusion tag (Cys-EGF) of 15 amino acids that could be used to conjugate therapeutic or imaging probes as done earlier with VEGF (11). In addition, the investigators also expressed EGF containing an N-terminal cysteine fusion tag (11). The dEGF and the EGF were then respectively labeled with radioactive technetium (^99m^Tc) to obtain [^99m^Tc]Cys-dEGF and [^99m^Tc]Cys-EGF. The biodistribution and imaging characteristics of the two molecules were subsequently investigated in xenograft tumor-bearing mice. It is pertinent to mention here that the imaging and biodistribution studies of only [^99m^Tc]Cys-dEGF are described in this chapter. Investigations performed with [^99m^Tc]Cys-EGF are described separately in MICAD (www.micad.nih.gov).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cys-tagged+EGF+synthesis)]

The Cys-dEGF was expressed in and purified from E. coli as described elsewhere to obtain Cys-tagged single-chain VEGF (Cys-scVEGF) (12). To label purified Cys-dEGF with ^99m^Tc, the protein was first incubated with an equimolar amount of dithiothreitol for 20 min at 25°C in 0.1 M Tris-HCl buffer (pH 8.0) to reduce all the sulfhydryl groups in the tagged protein (11, 12). The reduced protein was then labeled with ^99m^Tc as detailed for Cys-scVEGF (11). The radiolabeled Cys-dEGF (dEGF/Tc) was purified with size-exclusion chromatography using a PD-10 column, and the average yield of the labeled product was 45 ± 13% (n = 13 labeling reactions) as determined by the amount of ^99m^Tc eluting from the column (10). The radiochemical purity of dEGF/Tc was 90–95% as determined with instant thin-layer chromatography (ITLC) (10). The Rf value for the labeled protein on ITLC was not reported. Specific activity of dEGF/Tc was reported to be 5.92–10.36 MBq/70 fmol (0.13–0.28 mCi/70 fmol) (10).

To investigate the stability of dEGF/Tc, the labeled protein was injected into mice (n = 2 animals), and then the animals were euthanized 2 min later (10). Blood from the mice was collected and centrifuged to obtain plasma. The plasma was then incubated for 10, 20, and 75 min at 37°C, and the protein-bound radioactivity was determined with ITLC. The radioactivity was reported to be associated with the plasma protein fraction for at least 75 min under these conditions. Stability of dEGF/Tc was also investigated under in vitro conditions by incubating the labeled protein in phosphate-buffered saline (PBS) for up to 3 h at room temperature followed by ITLC and polyacrylamide gel analysis under denaturing conditions. dEGF/Tc was reported to be stable in PBS at room temperature for at least 3 h.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+Cys-EGF+in+vitro)]

In another study, Cys-EGF was reported to induce EGFR TK phosphorylation in F98/EGFR(F) cells (rat glioma cells transfected with the human EGFR gene) in a dose-dependent manner (10). Cys-dEGF was also reported to compete with an EGF-Shiga-like toxin subunit A conjugate (EGF-SLT (http://www.sibtech.com/?p=targeted_toxins)) for binding to the EGFR (10). EGF-SLT is extremely toxic to MDA23 1luc human breast cancer cells, and the ability of proteins to compete for binding with the EGFR was measured by counting the number of cells surviving after a 72-h exposure to EGF-SLT (1 nM) in the presence of an increasing concentration of Cys-EGF (0–25 nM). It was reported that cell survival increased with an increasing Cys-dEGF concentration under these experimental conditions, which indicates that Cys-dEGF protected the cells from EGF-SLT toxicity.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99m+Tc+Cys+EGF+rodentia)]

Levashova et al. studied the blood clearance and biodistribution of dEGF/Tc in mice (n = 4 animals) bearing MDA23 1luc cell tumors (10). The animals were injected with the radiotracer, and blood was collected at preselected time points for up to 60 min. More than 95% of the radioactivity was reported to clear from blood within 60 min. To determine biodistribution of the labeled protein, the animals were euthanized 3 h after administration of the tracer, all the major organs and the tumors were harvested, and radioactivity incorporated in the harvested organs was counted using a gamma counter. The radioactivity was reported to have accumulated primarily in the liver (24.5 ± 7.4% injected dose/gram tissue (% ID/g)) and kidneys (45.5 ± 1.4% ID/g). Compared with [^99m^Tc]Cys-EGF, both organs were reported to accumulate a higher amount of dEGF/Tc. Also, the outer edges and the center of each tumor were reported to have a similar accumulation of radioactivity after the dEGF/Tc treatment, indicating that the tracer was distributed throughout the tumor mass. No blocking studies were reported.

The accumulation of dEGF/Tc was investigated in mice bearing either orthotopic MDA23 1luc cell tumors or spontaneous lung carcinoma (10). The animals (n = 4 mice per model) were injected with the radiolabeled protein and imaged 1 h later with single-photon emission computed tomography (SPECT). Compared with the surrounding normal tissue, accumulation of radioactivity in the tumors was reported to be clearly evident in both tumor types. No blocking studies were reported.

Autoradiography of cryosections prepared from the MDA23 1luc tumors (n = 2 animals) immediately after SPECT imaging confirmed that accumulated radioactivity after the dEGF/Tc treatment was significantly higher in the tumors than in the normal muscle tissue. No blocking studies were reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99m+Tc+Cys+EGF+Non-Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99m+Tc+Cys+EGF+Non-Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99m+Tc+Cys+EGF+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Wu W.K., Tse T.T., Sung J.J., Li Z.J., Yu L., Cho C.H. (2009). Expression of ErbB receptors and their cognate ligands in gastric and colon cancer cell lines. Anticancer Res.
2 Schoenleber S.J., Kurtz D.M., Talwalkar J.A., Roberts L.R., Gores G.J. (2009). Prognostic role of vascular endothelial growth factor in hepatocellular carcinoma: systematic review and meta-analysis. Br J Cancer.
3 Balkwill F. (2009). Tumour necrosis factor and cancer. Nat Rev Cancer.
4 Wilkins-Port C.E., Ye Q., Mazurkiewicz J.E., Higgins P.J. (2009). TGF-beta1 + EGF-initiated invasive potential in transformed human keratinocytes is coupled to a plasmin/MMP-10/MMP-1-dependent collagen remodeling axis: role for PAI-1. Cancer Res.
5 Baselga J., Arteaga C.L. (2005). Critical update and emerging trends in epidermal growth factor receptor targeting in cancer. J Clin Oncol.
6 Varella-Garcia M., Mitsudomi T., Yatabe Y., Kosaka T., Nakajima E., Xavier A.C., Skokan M., Zeng C., Franklin W.A., Bunn P.A., Hirsch F.R. (2009). EGFR and HER2 genomic gain in recurrent non-small cell lung cancer after surgery: impact on outcome to treatment with gefitinib and association with EGFR and KRAS mutations in a Japanese cohort. J Thorac Oncol.
7 Chung K.Y., Shia J., Kemeny N.E., Shah M., Schwartz G.K., Tse A., Hamilton A., Pan D., Schrag D., Schwartz L., Klimstra D.S., Fridman D., Kelsen D.P., Saltz L.B. (2005). Cetuximab shows activity in colorectal cancer patients with tumors that do not express the epidermal growth factor receptor by immunohistochemistry. J Clin Oncol.
8 Bell D.W., Lynch T.J., Haserlat S.M., Harris P.L., Okimoto R.A., Brannigan B.W., Sgroi D.C., Muir B., Riemenschneider M.J., Iacona R.B., Krebs A.D., Johnson D.H., Giaccone G., Herbst R.S., Manegold C., Fukuoka M., Kris M.G., Baselga J., Ochs J.S., Haber D.A. (2005). Epidermal growth factor receptor mutations and gene amplification in non-small-cell lung cancer: molecular analysis of the IDEAL/INTACT gefitinib trials. J Clin Oncol.
9 Johns T.G., Perera R.M., Vernes S.C., Vitali A.A., Cao D.X., Cavenee W.K., Scott A.M., Furnari F.B. (2007). The efficacy of epidermal growth factor receptor-specific antibodies against glioma xenografts is influenced by receptor levels, activation status, and heterodimerization. Clin Cancer Res.
10 Levashova Z., Backer M.V., Horng G., Felsher D., Backer J.M., Blankenberg F.G. (2009). SPECT and PET imaging of EGF receptors with site-specifically labeled EGF and dimeric EGF. Bioconjug Chem.
11 Levashova Z., Backer M., Backer J.M., Blankenberg F.G. (2008). Direct site-specific labeling of the Cys-tag moiety in scVEGF with technetium 99m. Bioconjug Chem.
12 Backer M.V., Levashova Z., Patel V., Jehning B.T., Claffey K., Blankenberg F.G., Backer J.M. (2007). Molecular imaging of VEGF receptors in angiogenic vasculature with single-chain VEGF-based probes. Nat Med.